# [^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Pro^1^,Tyr^4^]Bombesin

Chemical name: | [^111^In-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid Pro^1^,Tyr^4^]Bombesin
Abbreviated name: | [^111^In-DOTA-Pro^1^,Tyr^4^]BN
Synonym: | ^111^In-BN, ^111^In-BBN
Agent Category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRP-R)
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure of [^111^In-DOTA-Pro^1^,Tyr^4^]BN. The possible ^111^In coordination configuration has not been established by experiments.. Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=55584176), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=2925&ordinalpos=5&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about BN and GRP.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Radiolabeled+Bombesin+analog+OR+(DOTA)-BN)]

[^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Pro^1^,Tyr^4^]Bombesin ([^111^In-DOTA-Pro^1^,Tyr^4^]BN) is a peptide analog of human gastrin-releasing peptide (GRP) conjugated with ^111^In, and it was developed for single-photon emission computed tomography (SPECT) imaging of tumors with overexpressed GRP receptors (GRP-R) (1). ^111^In is a gamma emitter with a physical half-life (t_½_) of 2.8 days.

The amphibian bombesin (BBN or BN), a peptide of 14 amino acids, is an analog of human GRP, a peptide of 27 amino acids, and binds to GRP-R with high affinity and specificity (2, 3). Both GRP and BN share an amidated C-terminus sequence homology of seven amino acids, -Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system (4, 5). They also act as potential growth factors for both normal and neoplastic tissues. Specific BN receptors (BN-R) have been identified in CNS and GI tissues and in a number of tumor cell lines. The BN-R superfamily includes at least four different subtypes, namely the GRP-R subtype (BB2), the neuromedin B receptor subtype (BB1), the BB3 subtype, and the BB4 subtype (8). Overexpression of GRP-R in various human tumors (e.g., breast, prostate, lung, colon, ovarian, and pancreatic cancers) provides opportunities to image tumors with the use of specific molecular imaging agents designed to target the GRP-R (3, 6-9).

There have been varying degrees of success in the development of GRP-R–targeted radiopharmaceuticals for diagnostic or therapeutic applications (9). Various BN analogs have been labeled with ^99m^Tc and ^111^In for SPECT imaging (13, 14). Despite some concern about the possible effect of BN to stimulate tumor growth, Breeman et al. (10) synthesized the BN-R agonist [^111^In-DTPA-Pro^1^,Tyr^4^]BN. The study reported that this agonist had a high specific localization in GRP-R–positive tissues and tumor. [^111^In-DTPA-Pro^1^,Tyr^4^]BN differs from native BN in that pGlu^1^ is replaced by DTPA-Pro^1^ and Leu^4^ is replaced by Tyr^4^. Breeman et al. (10) showed that this agonist was internalized by cells expressing GRP-R whereas the antagonist [^111^In-DTPA-Tyr^5^,D-Phe^6^]BN(5-13)NHEt was not. In another study, Breeman et al. (1) used the more stable DOTA chelator to prepare [^111^In-DOTA-Pro^1^,Tyr^4^]BN.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(Radiolabeled+Bombesin+analog+OR+(DOTA)-BN)+AND+synthesis)]

[DOTA-Pro^1^,Tyr^4^]BN was synthesized with the solid-phase method using the Fmoc strategy and Rink amide resin (10). The procedure of coupling of DOTA to [Pro^1^,Tyr^4^]BN was not described. Radiolabeling of [DOTA-Pro^1^,Tyr^4^]BN with ^111^In used the same procedure as described by de Jong et al. (11). Twenty μg peptide in 100 μl 0.2 M ammonium acetate (pH 5) was mixed with 1 mg gentisic acid in 83 μl 0.05 M acetic acid and ^111^In in 50 nM hydrochloric acid. The reaction mixture was heated at 100ºC for 25 min. The labeling efficiency was >95%, but it dropped to <95% when the ratio of radioactivity versus peptide exceeded 30 mBq ^111^In per nmol (0.81 mCi/nmol) of [DOTA-Pro^1^,Tyr^4^]BN. The specific activity was as high as 30 MBq/nmol (0.81 mCi/nmol). The radiochemical purity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DOTA)-BN))+AND+(in+vitro))]

Breeman et al. (1) studied the in vitro BN receptor binding and internalization of [^111^In-DOTA-Pro^1^,Tyr^4^]BN using membranes prepared from the GRP-R–positive AR42J rat pancreatic tumor cells. [^111^In-DTPA-Pro^1^,Tyr^4^]BN was used as the radioligand, and unlabeled [Tyr^4^]BN was used as the competitor. The inhibition concentration (IC_50_) value for [DOTA-Pro^1^,Tyr^4^]BN was 3–9 nM. In comparison, the IC_50_ for [Tyr^4^]BN was 1 nM. The binding values (% dose/mg protein) of [^111^In-DOTA-Pro^1^,Tyr^4^]BN were ~5.6% and ~22.2% at 5ºC and 37ºC, respectively, after 90 min of incubation (extrapolated from Figure 2B of Breeman et al. (1)). The internalization values of [^111^In-DOTA-Pro^1^,Tyr^4^]BN were 2.8% and 19.4% at 5ºC and 37ºC, respectively. In another study that used the GRP-R–positive CA20948 rat pancreatic tumor cells, the binding values of [^111^In-DOTA-Pro^1^,Tyr^4^]BN were ~5.6% and ~20.2% at 5ºC and 37ºC, respectively after 90 min of incubation (extrapolated from Figure 2A of Breeman et al. (1)). The internalization values of [^111^In-DOTA-Pro^1^,Tyr^4^]BN were 2.2% and 20.0% at 5ºC and 37ºC, respectively, after 90 min of incubation. No blocking study was reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DOTA)-BN))+AND+(rodentia))]

The biodistribution of [^111^In-DOTA-Pro^1^,Tyr^4^]BN was performed in three male rats (210–260 g) (1). The dose of [^111^In-DOTA-Pro^1^,Tyr^4^]BN for each rat was not reported. The rats were euthanized 24 hr after administration. Nonspecific uptake of radioactivity was determined by coinjection of a GRP receptor–blocking dose of 0.1 mg [Tyr^4^]BN. The difference between total uptake and nonspecific uptake represented specific localization of [^111^In-DOTA-Pro^1^,Tyr^4^]BN to the GRP-R. The highly GRP-R–positive pancreas had the highest specific radioactivity level of 1.2% injected dose per gram (% ID/g). In comparision, [^111^In-DTPA-Pro^1^,Tyr^4^]BN had a pancreas radioactivity level of 0.9% ID/g. The pancreas/blood radioactivity level ratio was 1,269. In comparison, the pancreas/blood ratio for [^111^In-DTPA-Pro^1^,Tyr^4^]BN was 526. Other GRP-R–positive tissues with significant specific radioactivity levels were the antrum, fundus, jejunum, colon, cecum, and adrenal and pituitary glands. Other GRP-R–negative organs had insignificant specific radioactivity levels. The kidney/blood ratio was 693 (extrapolated from Figure 4 in Breeman et al. (1),) the spleen/blood ratio was 24.3, and the liver/blood ratio was 25.6. Gamma imaging in a rat bearing the AR42J subcutaneous tumor at 24 h after injection showed accumulation of radioactivity in the kidneys, and the tumor was clearly visualized.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DOTA)-BN))+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DOTA)-BN))+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((Radiolabeled+Bombesin+analog+OR+(DOTA)-BN))+AND+(humans))]

No publication is currently available.

## References

1 Breeman W.A., de Jong M., Erion J.L., Bugaj J.E., Srinivasan A., Bernard B.F., Kwekkeboom D.J., Visser T.J., Krenning E.P. (2002). Preclinical comparison of (111)In-labeled DTPA- or DOTA-bombesin analogs for receptor-targeted scintigraphy and radionuclide therapy. J Nucl Med.
2 Smith C.J., Gali H., Sieckman G.L., Higginbotham C., Volkert W.A., Hoffman T.J. (2003). Radiochemical investigations of (99m)Tc-N(3)S-X-BBN[7-14]NH(2): an in vitro/in vivo structure-activity relationship study where X = 0-, 3-, 5-, 8-, and 11-carbon tethering moieties. Bioconjug Chem.
3 Ma L., Yu P., Veerendra B., Rold T.L., Retzloff L., Prasanphanich A., Sieckman G., Hoffman T.J., Volkert W.A., Smith C.J. (2007). In Vitro and In Vivo Evaluation of Alexa Fluor 680-Bombesin[7-14]NH(2) Peptide Conjugate, a High-Affinity Fluorescent Probe with High Selectivity for the Gastrin-Releasing Peptide Receptor. Mol Imaging.
4 Mantey S., Frucht H., Coy D.H., Jensen R.T. (1993). Characterization of bombesin receptors using a novel, potent, radiolabeled antagonist that distinguishes bombesin receptor subtypes. Mol Pharmacol.
5 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
6 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
7 Biddlecombe G.B., Rogers B.E., de Visser M., Parry J.J., de Jong M., Erion J.L., Lewis J.S. (2007). Molecular imaging of gastrin-releasing peptide receptor-positive tumors in mice using 64Cu- and 86Y-DOTA-(Pro1,Tyr4)-bombesin(1-14). Bioconjug Chem.
8 Nock B., Nikolopoulou A., Chiotellis E., Loudos G., Maintas D., Reubi J.C., Maina T. (2003). [99mTc]Demobesin 1, a novel potent bombesin analogue for GRP receptor-targeted tumour imaging. Eur J Nucl Med Mol Imaging.
9 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
10 Breeman W.A., Hofland L.J., de Jong M., Bernard B.F., Srinivasan A., Kwekkeboom D.J., Visser T.J., Krenning E.P. (1999). Evaluation of radiolabelled bombesin analogues for receptor-targeted scintigraphy and radiotherapy. Int J Cancer.
11 de Jong M., Bakker W.H., Krenning E.P., Breeman W.A., van der Pluijm M.E., Bernard B.F., Visser T.J., Jermann E., Behe M., Powell P., Macke H.R. (1997). Yttrium-90 and indium-111 labelling, receptor binding and biodistribution of [DOTA0,d-Phe1,Tyr3]octreotide, a promising somatostatin analogue for radionuclide therapy. Eur J Nucl Med.